# ^99m^Tc-Labeled doxorubicin

Chemical name: | ^99m^Tc-Labeled doxorubicin
Abbreviated name: | ^99m^Tc-doxorubicin
Synonym:
Agent Category: | Compounds
Target: | DNA (topoisomerase II enzyme)
Target Category: | Nucleic acids
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Structure of doxorubicin in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance/?term=doxorubicin).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=doxorubicin%20and%20molecular%20imaging%20and%20treatment)]

Molecular imaging is considered to be a decision-making tool throughout the drug discovery and initial stages of clinical trials (1, 2). Molecular imaging techniques have been used to validate the potential drug targets, determine the drug pharmacokinetics and biodistribution, and assess the drug–target interaction (3). One notable example is the phase 0 clinical trial, which has been developed in response to the exploratory Investigational New Drug (IND) guidance of the United States Food and Drug Administration (1, 4). Phase 0 clinical trials perform first-in-human testing of IND drugs at microdoses (<100 ug) and allow the demonstration of drug–target effects and assessment of pharmacokinetic–pharmacodynamic relationships in humans earlier in clinical development (2, 3). Phase 0 trials are expected to reduce the high failure rate of new drug candidates in clinical trials and to decrease the prolonged timeline and high cost due to the low predictability of toxicity and efficacy with traditional preclinical studies. The drug and target information in these studies is obtained by directly labeling the drugs themselves and/or by imaging the drug targets with specific molecular probes. On the other hand, some well-studied, clinically used drugs have been explored as molecular imaging agents for tumor detection and other purposes. These studies take advantage of the fact that these drugs are already well understood in terms of their targeting, pharmacokinetics, toxicity, and other characteristics. Examples include the studies performed by Kumar et al., who tested the feasibility of doxorubicin as an imaging agent for tumor detection (5).

Doxorubicin is a well-investigated anthracycline antibiotic and widely used in cancer chemotherapy (6). The planar aromatic chromophore portion of doxorubicin intercalates between two base pairs of DNA, while the six-membered daunosamine sugar sits in the minor groove and interacts with the flanking base pairs immediately adjacent to the intercalation site (6, 7). The doxorubicin–DNA intercalation inhibits the progression of the enzyme topoisomerase II and stabilizes the topoisomerase II complex after it breaks the DNA chain; this prevents the DNA double helix from being resealed and thereby stops the process of replication. It is estimated that several thousand doxorubicin analogs have been synthesized (8). This chapter summarizes the data obtained in studies of ^99m^Tc-doxorubicin performed by Kumar et al. (5).

### Related Resource Links:

Drug information of doxorubicin (http://www.nlm.nih.gov/medlineplus/druginfo/meds/a682221.html) in MedlinePlus

Doxorubicin-related clinical trials (http://clinicaltrials.gov/ct2/results?term=doxorubicin&Search=Search) in Clinicaltrials.gov

Drugs with doxorubicin as the active ingredient (http://www.accessdata.fda.gov/scripts/cder/drugsatfda/index.cfm) in Drug@FDA

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22432523)]

Doxorubicin is commercially available. Fresh pertechnetate (^99m^TcO_4_^–^) eluted from a molybdenum-99/technetium-99m column generator was used for the labeling procedures (5). Variable concentrations (20, 50, 100, 200, 400, and 1,000 μg) of stannous chloride (SnCl_2_·2H_2_O), different pH conditions (pH 2–9), and variable incubation times (5, 10, 20, and 30 min) were tested. A mixture was first prepared by dissolving doxorubicin in water, followed by addition of a standardized concentration of stannous chloride dihydrate (pH 6.0). Radioactive pertechnetate (~40.0 MBq, ~1.08 mCi) was then added to the mixture and incubated for 15 min to generate ^99m^Tc-doxorubicin.

The best labeling efficiency was achieved at pH 6.0, and the efficiency deteriorated with pH values in the alkaline range. An incubation time of 10–20 min was found to be adequate for complete labeling. The ^99m^Tc-doxorubicin preparation remained stable (>95% labeling efficiency) for up to 24 h, as only a small fraction of the preparation (1%–2%) degraded over a period of 24 h. The lipophilicity was found to be 16.41 ± 0.33% (organic/aqueous partition coefficient). The radiochemical purity and specific activity were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22432523)]

The serum stability was evaluated by incubating ^99m^Tc-doxorubicin in normal human serum for different times at 37°C (5). The ^99m^Tc-doxorubicin remained >95% intact up to 24 h in serum. Only 2%–3% degradation was noticed. The plasma protein binding was determined to be 81.17 ± 1.33% (protein-bound radioactivity in total radioactivity) after incubation of ^99m^Tc-doxorubicin in human plasma for 1 h at 37°C.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22432523)]

Blood kinetics of ^99m^Tc-doxorubicin was studied in an adult rabbit after intravenous (dorsal ear vein) injection of ~20.0 MBq (0.54 mCi) ^99m^Tc-doxorubicin (5). The results showed that ^99m^Tc-doxorubicin had a biexponential clearance pattern. Nearly half (50%) of the radiotracer cleared from the circulation at 1.2 h, and only 0.97% of the tracer activity remained in blood at 24 h. The clearance times (t_1/2_) by fast and slow components were determined to be 2.4 ± 0.2 h and 13.3 ± 0.3 h, respectively.

The biodistribution studies were carried out in male Wistar rats (n = 4) after injection of 7.4 MBq (0.2 mCi) ^99m^Tc-doxorubicin (5). The activity in different organs was measured ex vivo and expressed as percentage of injected dose per gram tissue (% ID/g). The maximum uptake of the radiotracer was seen in kidneys (3.1% ID/g) at 1 h, followed by spleen (1.3% ID/g) and liver (0.8% ID/g). The activity in lungs washed out very rapidly.

The tumor animal model was established by injecting Ehrlich ascites tumor cells into the right thigh region of Balb/c mice (number not reported), and the tumor was allowed to grow to ~1 cm in diameter. Imaging was performed with a single-head gamma camera at different times after injection of 7.4 MBq (0.2 mCi) ^99m^Tc-doxorubicin. Semiquantitative analysis showed that the tumor/background (contralateral thigh) ratio was 2.5, 3.0, and 3.3 at 1.5, 3, and 4 h after injection, respectively. No blocking studies or other studies of specific binding to DNA were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term)]

No references are currently available.

## References

1 Gomes C.M., Abrunhosa A.J., Ramos P., Pauwels E.K. (2011). Molecular imaging with SPECT as a tool for drug development. Adv Drug Deliv Rev.
2 Sugiyama Y., Yamashita S. (2011). Impact of microdosing clinical study -- why necessary and how useful?. Adv Drug Deliv Rev.
3 Murgo A.J., Kummar S., Rubinstein L., Gutierrez M., Collins J., Kinders R., Parchment R.E., Ji J., Steinberg S.M., Yang S.X., Hollingshead M., Chen A., Helman L., Wiltrout R., Tomaszewski J.E., Doroshow J.H. (2008). Designing phase 0 cancer clinical trials. Clin Cancer Res.
4 Kummar S., Rubinstein L., Kinders R., Parchment R.E., Gutierrez M.E., Murgo A.J., Ji J., Mroczkowski B., Pickeral O.K., Simpson M., Hollingshead M., Yang S.X., Helman L., Wiltrout R., Collins J., Tomaszewski J.E., Doroshow J.H. (2008). Phase 0 clinical trials: conceptions and misconceptions. Cancer J.
5 Kumar P., Singh B., Sharma S., Ghai A., Chuttani K., Mishra A.K., Dhawan D., Mittal B.R. (2012). Preclinical evaluation of [99m]Tc-labeled doxorubicin as a potential scintigraphic probe for tumor imaging. Cancer Biother Radiopharm.
6 Dickey J.S., Rao V.A. (2012). Current and proposed biomarkers of anthracycline cardiotoxicity in cancer: emerging opportunities in oxidative damage and autophagy. Curr Mol Med.
7 Binaschi M., Bigioni M., Cipollone A., Rossi C., Goso C., Maggi C.A., Capranico G., Animati F. (2001). Anthracyclines: selected new developments. Curr Med Chem Anticancer Agents.
8 Minotti G., Menna P., Salvatorelli E., Cairo G., Gianni L. (2004). Anthracyclines: molecular advances and pharmacologic developments in antitumor activity and cardiotoxicity. Pharmacol Rev.